# 2-[(4-{[(2-amino-4-oxohydropteridin-7yl)methyl]amino}phenyl) carbonylamino]-4-{N-[(4-[^18^F]-fluorophenyl)carbonylamino] carbamoyl}butanoic acid

Chemical name: | 2-[(4-{[(2-Amino-4-oxohydropteridin-7yl)methyl]amino}phenyl) carbonylamino]-4-{N-[(4-[^18^F]fluorophenyl)carbonylamino] carbamoyl}butanoic acid
Abbreviated name: | [^18^F]-Folate-1
Synonym: | [^18^F]-4-fluorobenzenecarbohydrazide-folate; [^18^F]-1; [^18^F]-6
Agent Category: | Compound
Target: | Folate receptor
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on above structure for information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=folate%20receptor%20imaging&cmd=DetailsSearch)]

Folic acid (FA; also known as folate or vitamin B_9_) is a water-soluble vitamin that is required for the synthesis and repair of cellular DNA. FA also acts as a cofactor for many biological reactions and has an important role in cell maintenance and proliferation. Although the folate receptor (FR) is expressed at low levels in normal cells, this receptor is known to be upregulated in cancers such as those of the ovary, lung, breast, brain, colon, and the hematopoietic lineage cells (1). Therefore, the FR system has been targeted with radiolabeled folate and its derivatives, such as ^67^Ga-deferoxamine (DF)-folate, ^111^In-diethylenetriamine pentaacetic acid-folate, ^99m^Tc-mercaptoacetyldiglycine-folate-methotrexate, etc., for the noninvasive detection of malignancies with single-photon emission computed tomography (2). Mathias et al. showed that ^66/67^Ga-DF-folate can be used with positron emission tomography (PET) for the imaging of FR-positive cancerous tumors in mice (3). However, although these tracers could detect the FR-rich tumors, they were deemed unsuitable for imaging lesions in the abdominal regions because high levels of radioactivity were observed to accumulate in the liver and intestines of the animals (4). In addition, ^66/67^Ga-labeled tracers are known to produce low-resolution images because they generate high positron energy (4.15 MeV and 1.89 MeV for ^66^Ga and ^67^Ga, respectively. ^67^Ga-labeled agents are used for single photon emission computed tomography imaging) compared to ^18^F (0.64 MeV), which generates superior images and is often used to radiolabel PET imaging agents in the clinic (4). In another study, it was shown that ^18^F-fluorobenzylamine derivatives of folate could detect tumors that had a high expression of FR, but the radioactivity from these labeled compounds accumulated mainly at the rim of the tumor, and large amounts of the label were retained in the liver and intestines of the animals (4, 5).

In an ongoing effort to generate radiolabeled agents for the imaging of tumors that express high levels of FRs that would be superior to those developed and evaluated earlier, a ^18^F-fluorobenzene derivative of folic acid ([^18^F]-folate-1), a pyridinecarbohydrazide-folate derivative of folic acid ([^18^F]-folate-2), a ^18^F-fluorobenzene/methotrexate (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=78794e3d-f293-4eeb-22ac-8f536d5947eb) (MTX) conjugate of folic acid ([^18^F]-folate-MTX-8), and a ^18^F-pyridinecarbohydrazide-folate/methotrexate conjugate of folic acid ([^18^F]-folate-MTX-9) have been synthesized (2). The biodistribution of these tracers was investigated in healthy mice. On the basis of results obtained from these studies, [^18^F]-folate-1 was evaluated for the PET imaging of human KB cell line (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-17&Template=cellBiology) xenograft tumors (have a high expression of FR) in mice. This chapter describes the results obtained with [^18^F]-folate-1. Separate chapters in MICAD (http://www.micad.nih.gov/) discuss the studies performed with [^18^F]-folate-2 (6), [^18^F]-folate-MTX-8 (7), and [^18^F]-folate-MTX-9 (8).

### Related Resource Links

FR-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Folate+receptor+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Adult human FR protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_016724.2)

Human FR gene (http://www.ncbi.nlm.nih.gov/gene/2348) (Gene ID: 2348)

FR clinical trials (http://clinicaltrials.gov/ct2/results?term=folate+receptor+AND+targeted+AND+cancer)

FR in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/136430) database

FR pathway in Kyoto Encyclopedia of Genes and Genomes (KEGG) (http://www.genome.jp/dbget-bin/www_bget?hsa:2348+hsa:2350+hsa:2352+hsa:390243)

Folic acid information on Dailymed site (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=ff80ef4d-e04c-9f83-2b56-cccc30028f72)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20synthesis&cmd=DetailsSearch)]

Folate-1 was synthesized with hydrazide-folate and 2,5-dioxoazolidinyl 4-fluorobenzoate in presence of triethylamine and the ^18^F labeling of folate-1 has been detailed elsewhere (9). The total time of synthesis was ~45 min, and the radiochemical yield and radiochemical purity of the final product were >80% (based on the initial ^18^F concentration) and >97% (without high-performance liquid chromatographic purification), respectively. The specific activity of the final product was reported to be >11.11 MBq/μmol (300 mCi/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20in%20vitro&cmd=DetailsSearch)]

Using an n-octanol-water mixture (pH 7.3), the partition coefficient of [^18^F]-folate-1 was determined to be 0.38 ± 0.02, indicating that the labeled compound had low lipophilicity (9).

[^18^F]-Folate-1 was reported to be stable in human plasma for at least 4 h at 37°C (data not presented) (9).

The FR binding affinity of [^18^F]-folate-1 was determined to be 13.08 ± 0.83 nM with a saturation assay using KB cell membranes (9). A cell internalization assay of [^18^F]-folate-1 with KB cells (using an acidic buffer, pH not mentioned) showed that 25.85 ± 0.95% of the tracer was internalized by the cells within 20 min at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]-folate-1 was studied in normal Balb/c mice as described by al Jammaz et al. (2). The animals (n = 4 mice/time point) were injected with 749 kBq (20 μCi) of the tracer through the tail vein and euthanized at 10, 60, and 120 min postinjection (p.i.) to determine the amount of radioactivity accumulated in the various organs. All data were presented as percent of injected dose per gram tissue (% ID/g). A rapid clearance of radioactivity from the blood was observed (4.41 ± 0.60% ID/g at 10 min p.i., 2.55 ± 1.50% ID/g at 60 min p.i., and 1.13 ± 0.51% ID/g at 120 min p.i.). High levels of the label were observed in the kidneys (22.50 ± 4.42% ID/g at 10 min p.i. and 17.88 ± 0.10% ID/g at 120 min p.i.) and the intestine (5.95 ± 2.11% ID/g at 10 min p.i. and 5.86 ± 0.26% ID/g at 120 min p.i.) of these animals. In the liver the amount of label decreased from 7.52 ± 1.43% ID/g at 10 min p.i. to 1.02 ± 0.61% ID/g at 60 min p.i. and to 0.32 ± 0.12% ID/g at 120 min p.i. indicating that the tracer was excreted through the urinary and the hepatobiliary routes. A similar trend of tracer uptake in the various organs was also observed with [^18^F]-folate-2 (for details, see Chopra (6)).

The biodistribution of [^18^F]-folate-1 was also investigated in nude mice (n = 4 animals) bearing KB cell tumors. The animals were injected with the radiotracer as described above and euthanized at 60 min p.i (2). The uptake of radioactivity in the various organs of the mice was similar to that observed earlier (see above), and the amount of label in the tumor was 5.94 ± 1.16% ID/g at 60 min p.i. The tumor/blood (T/B) and tumor/muscle (T/M) ratios at 60 min p.i. were 6.39 and 25.83, respectively. The T/B and T/M ratios at 60 min p.i. with [^18^F]-folate-2 were 14.70 and 28.70, respectively (see Chopra for details (6)). For blocking studies, the mice were injected with 100 μg (0.22 μmol) FA 10 min before the administration of [^18^F]-folate-1, and the rodents were treated as described above (2). Under these conditions, the uptake of radioactivity in the tumors was reduced significantly (0.74 ± 0.17% ID/g, P <0.05); the kidneys, liver, and intestines (among these organs only the kidneys and the liver have an above normal expression of the FR) also showed a significantly (P < 0.05) reduced accumulation of the label. With [^18^F]-folate-2, the uptake in the tumor at 60 min p.i. was reduced to 0.66 ± 0.10% ID/g, and the amount of label in the kidneys, liver, and intestines was also reduced significantly (P < 0.05). This indicated that both [^18^F]-folate-1 and [^18^F]-folate-2 had a high binding specificity for the FR.

Table: Tumor Uptake and Tumor/Blood and Tumor/Muscle Ratios of different ^ 18 ^ F-Labeled Folate

Tracer | Tumor Uptake (% ID/g) | | Ratio (No Folate Pre-treatment)
Tracer | No Folate Pre-treatment | With Folate (100 μg) Pre-treatment | Tumor/blood | Tumor/Muscle
[ ^ 18 ^ F]-Folate-1 | 5.94 ± 1.16 | 0.74 ± 0.17 | 6.39 | 25.83
[ ^ 18 ^ F]-Folate-2 | 5.74 ± 0.16 | 0.66 ± 0.10 | 14.72 | 28.70

From this study, the investigators concluded that [^18^F]-folate-2 was probably superior to [^18^F]-folate-1 for the imaging of FR-rich tumors (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Xia W., Low P.S. (2010). Folate-targeted therapies for cancer. J Med Chem.
2 Al Jammaz I., Al-Otaibi B., Amer S., Okarvi S.M. (2011). Rapid synthesis and in vitro and in vivo evaluation of folic acid derivatives labeled with fluorine-18 for PET imaging of folate receptor-positive tumors. Nucl Med Biol.
3 Mathias C.J., Lewis M.R., Reichert D.E., Laforest R., Sharp T.L., Lewis J.S., Yang Z.F., Waters D.J., Snyder P.W., Low P.S., Welch M.J., Green M.A. (2003). Preparation of 66Ga- and 68Ga-labeled Ga(III)-deferoxamine-folate as potential folate-receptor-targeted PET radiopharmaceuticals. Nucl Med Biol.
4 Sega E.I., Low P.S. (2008). Tumor detection using folate receptor-targeted imaging agents. Cancer Metastasis Rev.
5 Bettio A., Honer M., Muller C., Bruhlmeier M., Muller U., Schibli R., Groehn V., Schubiger A.P., Ametamey S.M. (2006). Synthesis and preclinical evaluation of a folic acid derivative labeled with 18F for PET imaging of folate receptor-positive tumors. J Nucl Med.
6 Chopra, A., 2-[(4-{[(2-amino-4-oxohydropteridin-7yl)methyl]amino}phenyl) carbonylamino]-4-{N-[(4-[18F]-fluorophenyl)carbonylamino] carbamoyl}butanoic acid. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
7 Chopra, A., 2-[(4-{[(2-amino-4-oxohydropteridin-7yl)methyl]amino}phenyl) carbonylamino]-4-{N-[(2-[18F]-fluoro(4-pyridyl))carbonylamino] carbamoyl}butanoic acid. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
8 Chopra, A., 2-[18F]Fluoropyridine-4-carbohydrazide-methotrexate (9). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Jammaz I.A., Otaibi B.A., Okarvi S., Amartey J.K. (2006). Novel synthesis of [18F]-fluorobenzene and pyridinecarbohydrazide-folates as potential PET radiopharmaceuticals. Journal of Labelled Compounds and Radiopharmaceuticals.